# Polyethylene glycol–coated and folic acid–conjugated superparamagnetic iron oxide nanoparticles

Chemical name: | Polyethylene glycol–coated and folic acid–conjugated superparamagnetic iron oxide nanoparticles
Abbreviated name: | SPIO-PEG-FA
Synonym: | SPIO-PEG_(2000)_-FA, SPIO-PEG_(400)_-FA
Agent Category: | Nanoparticles
Target: | Folate receptor (FA)
Target Category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Superparamagnetic iron oxide (SPIO)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/sites/entrez?db=protein&cmd=search&term=folate+receptor), nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?db=nucleotide&cmd=search&term=folate+receptor) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=search&term=folate+receptor) for more information about folate receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=superparamagnetic%20iron%20oxide%20and%20folate%20receptor)]

The polyethylene glycol (PEG)–coated and folic acid (FA)–conjugated superparamagnetic iron oxide (SPIO) nanoparticles (SPIO-PEG-FA) were developed by Chen et al. as a magnetic resonance imaging (MRI) contrast agent for molecular imaging of tumors overexpressing folate receptor (1).

MRI is an imaging modality that is used to construct images of the nuclear magnetic resonance (NMR) signal, primarily from the hydrogen atoms in an object. The image contrast is achieved by the differences in the NMR signal intensity in different areas within the object; the NMR signal intensity depends on the nuclear density (proton spins), the relaxation times (T_1_, T_2_, and T_2_*), and the magnetic environment of the tissues. Contrast agents serve to enhance the image contrast and thus improve the sensitivity and specificity of MRI in mapping information from tissues (2, 3). SPIO nanoparticles comprise a class of novel MRI contrast agents that are composed of a ferric iron (Fe^3+^) and ferrous iron (Fe^2+^) core and a layer of dextran or other polysaccharide coating (2, 4). The iron nanoparticles have very large magnetic moment, which leads to local magnetic field inhomogeneity. Consequently, the NMR signal intensity is significantly decreased, appearing dark on T_2_- and T_2_*-weighted images. On the basis of molecular diameter, SPIO nanoparticles are commonly classified as oral SPIO (300 nm–3.5 µm), polydisperse SPIO (PSPIO, 50–150 nm), and ultrasmall SPIO (USPIO, <50 nm). In addition, USPIO nanoparticles with an iron oxide core monocrystalline in nature are referred to as monocrystalline iron oxide nanoparticles (MION), and MION with a chemically cross-linked and aminated polysaccharide shell are called cross-linked iron oxide nanoparticles (CLIO) (5).

Clinically, SPIO nanoparticles are predominantly used as a T_2_/T_2_* contrast agent, though it could shorten both T_1_ and T_2_/T_2_* relaxation processes. Successful application of a SPIO-based contrast agent is dependent on its size, size distribution, shape, magnetic susceptibility, and surface modification. In vivo, nonspecific SPIO nanoparticles are mainly captured by the reticuloendothelial system (RES), and they are more suitable for liver, spleen, and lymph node imaging (6). Because of their long plasma half-life (hours), SPIO are also used as blood pool agents in magnetic resonance angiography (7). Accumulation of the nonspecific SPIO in tumors relies on the enhanced permeation and retention effect defined by the tumor's leaky vasculature and poor lymphatic drainage. Specific SPIO nanoparticles are developed by conjugating the respective targeting agents directly onto the SPIO surface or onto its hydrophilic coating. Specific accumulation of the agents at the disease-specific sites is achieved because of the target overexpression (often cell surface receptors) and receptor-mediated endocytosis and recycling (2, 3). The signal decrease is much more obvious in the lesions than in the surrounding normal tissues. An inverse strategy of SPIO-based molecular imaging is also applied in some studies by designing molecules that bind to targets expressing on normal tissues. This strategy has been proven to be valuable in imaging pancreatic ductal adenocarcinomas and hepatocellular carcinomas by targeting the receptors of bombesin, cholecystokinin, or asialoglycoprotein in normal tissue (8, 9). By decreasing the T_2_ signal of the normal tissue surrounding a tumor more than that of the tumor, the contrast between healthy and tumor tissues is enhanced.

Chen et al. developed a SPIO-based MRI contrast agent by immobilizing the PEG and FA on the surface of SPIO nanoparticles (SPIO-PEG-FA) (1). PEG was used to increase the blood circulation time of the nanoparticles, and FA was designed to target the cancer cells and to increase the cell internalization via the folate receptor–mediated endocytosis and recycling. The folate receptor is a high-affinity, glycosylphosphatidylinositol-anchored protein that is overexpressed in various types of human tumors. Folate is vital for the rapid proliferation of tumor cells. In contrast, nonproliferating healthy cells are severely restricted in possessing folate receptors. Folate receptors provide highly selective sites that differentiate tumor cells from normal cells. In addition, folate has no immunotoxicity. Because of these unique features, folate conjugates have been intensively investigated as drugs, drug carriers, and imaging agents (10-12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=superparamagnetic%20iron%20oxide%20and%20folate%20receptor%20and%20synthesis)]

Synthesis of the SPIO-PEG-FA nanoparticles can be divided into four consecutive steps: synthesis of SPIO, synthesis of PEG monotosylate (PEG-OTs), SPIO coating and FA conjugation (1). The SPIO nanoparticles were synthesized by dissolving FeCl_3_ and FeCl_2_·4H_2_O in the HCl solution, and the resulting solution was added to a solution of NaOH. The precipitate was isolated with centrifugation, dispersed in deoxygenated water, and then mixed with oleic acid. The SPIO product was extracted with toluene. The PEG-OTs was synthesized by mixing toluene-4-sulfonyl chloride with triethylamine and PEG_(400)_ or PEG_(2000)_. The mixture was stirred for 24 h at room temperature and then washed with deoxygenated water and hexane sequentially. The yields of PEG_(400)_-OTs and PEG_(2000)_-OTs were 94.41% and 92.6%, respectively. To coat the SPIO with PEG, a mixture of toluene, methanol, (3-aminopropyl)trimethoxy silane, and SPIO was prepared and stirred rigorously for 6 h under N_2_. PEG_(400)_-OTs or PEG_(2000)_-OTs was then added to the mixture, followed by stirring for 12 h at room temperature. The precipitate was isolated with centrifugation and dispersed in deoxygenated water to provide the corresponding SPIO-PEG-NH_2_. To conjugate FA onto the surface of SPIO-PEG-NH_2_, FA was first mixed with 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide in dimethyl sulfoxide (stirring for 0.5 h at room temperature). The SPIO-PEG_(400)_-NH_2_ or SPIO-PEG_(2000)_-NH_2_ was then added to the mixture and stirred for 24 h. The product (SPIO-PEG-FA) was purified with dialysis.

Chen et al. characterized the SPIO-PEG-FA nanoparticles with various techniques (1). X-ray diffraction (XRD) showed that the SPIO-PEG_(400)_-FA and the SPIO-PEG_(2000)_-FA had mean diameters of 30 and 32 nm, respectively. Both SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA showed high saturation magnetization at 298 K (62 and 65 emu/g Fe, respectively). Thermal gravimetric analysis demonstrated that the main weight loss (changes in weight in relation to change in temperature), observed at >400°C, was 57% for the SPIO-PEG_(400)_-FA and 60% for the SPIO-PEG_(2000)_-FA. With Fourier transform infrared spectroscopy, the characteristic spectra of folic acid at ranges of 1,600–1,610 cm^-1^ and 1,680–1,690 cm^-1^ were observed only in the spectra of the SPIO-PEG-FA. Imaging with a transmission electron microscope demonstrated that the nanoparticles exhibited a well dispersed property, and the SPIO nanoparticle diameters of the SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA were 3.8 ± 0.8 nm and 4.1 ± 0.5 nm (n = 200 particles), respectively, values similar to the results obtained from the XRD analysis (3.4 nm). In aqueous solution at 37.0 ± 0.1°C and 20 MHz, the r_1_ relaxivity values were 4.7 ± 0.2 and 5.9 ± 0.1 mM^-1^s^-1^, and the r_2_ values were 117.3 ± 0.3 and 105.7 ± 0.3 mM^-1^s^-1^ for the SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA, respectively. In the 3.0 T field strength, the r_1_ relaxivity values were 11.9 ± 0.5 and 11.8 ± 0.8 mM^-1^s^-1^, and the r_2_ values were 200.4 ± 3.6 and 194.8 ± 0.3 mM^-1^s^-1^ for the SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA, respectively. Two pulse sequences were used: T_1_-weighted sequence: TE = 150 ms, TR = 100–2,000 ms; T_2_-weighted sequence: TR = 750 ms, TE = 50–300 ms. The field of view was set at 24 with 10 excitations. Both SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA were well dispersed in phosphate-buffered saline at pH 7.4 as well as in the pH range from 1 to 10, with no aggregation for at least 3 months.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=superparamagnetic%20iron%20oxide%20and%20folate%20receptor%20and%20in%20vitro)]

Because the nonspecific SPIO-based nanoparticles are usually captured in vivo in the RES, Chen et al. analyzed the in vitro cell uptake of the SPIO-PEG-FA nanoparticles by macrophages using the macrophage cell line RAW264.7 (1). After incubation of the cells with the nanoparticles for 24 h, only a slight cell uptake was observed as the nanoparticle concentration increased to 0.8 mg Fe/well (10^6^ cells) for both SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA. No morphological change of the cells was observed.

The binding affinity of SPIO-PEG_(400)_-FA was determined with competition binding assay in folate receptor-expressing KB cells (human nasopharyngeal epidermal carcinoma cells) (1). FITC-Labeled PEG-FA (PEG-FA-FITC) was used as a competitor for specific receptor binding. Flow cytometric analysis showed that both SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA bound specifically with the cells. The binding of PEG-FA-FITC was blocked by pretreatment of the cells with SPIO-PEG_(400)_-FA.

The cell internalization was confirmed with a 3.0-T MRI imager. The signal intensity from the cells incubated with SPIO-PEG-FA nanoparticles was clearly decreased when compared with KB cells alone. On the contrary, no difference in the signal intensity was detected when the HT-1080 cells incubated with SPIO-PEG-FA were compared with HT-1080 cells alone. HT-1080 cells (human fibrosarcoma cells) do not express folate receptors.

The cytotoxicity of the SPIO-PEG-FA nanoparticles was analyzed with MTT (3-(4,5-dimethylthiazol-2-yl)-2,5-diphenyltetrazolium bromide) cell viability assay after incubation of the KB and HT-1080 cells with the SPIO-PEG-FA nanoparticles. After 48 h incubation, no inhibition of the cell growth was detected for either KB or HT-1080 cells with up to 0.4–0.6 mmol Fe.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=superparamagnetic%20iron%20oxide%20and%20folate%20receptor%20and%20animal)]

MRI studies were performed in SCID mice bearing both KB and HT-1080 tumor xenografts (n = 5 mice) (1). At 2 h after intravenous injection of the SPIO-PEG-FA solution (40 µmol/kg), the MRI was performed with a 3.0-T MRI imager and T_2_-weighted spin-echo sequence (TR/TE = 2,000/60). Comparison of the images before and after injection showed that the average intensity of the KB tumor xenografts decreased ~20% and ~25% for SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA, respectively. On the contrary, a slight increase of the signal intensity was detected in the HT-1080 tumor xenografts for both SPIO-PEG_(400)_-FA and SPIO-PEG_(2000)_-FA. Biodistribution and blocking studies were not performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Chen T.J., Cheng T.H., Hung Y.C., Lin K.T., Liu G.C., Wang Y.M. (2008). Targeted folic acid-PEG nanoparticles for noninvasive imaging of folate receptor by MRI. J Biomed Mater Res A.
2 Islam T., Josephson L. (2009). Current state and future applications of active targeting in malignancies using superparamagnetic iron oxide nanoparticles. Cancer Biomark.
3 Corot C., Robert P., Idee J.M., Port M. (2006). Recent advances in iron oxide nanocrystal technology for medical imaging. Adv Drug Deliv Rev.
4 Bulte J.W., Kraitchman D.L. (2004). Iron oxide MR contrast agents for molecular and cellular imaging. NMR Biomed.
5 Di Marco M., Sadun C., Port M., Guilbert I., Couvreur P., Dubernet C. (2007). Physicochemical characterization of ultrasmall superparamagnetic iron oxide particles (USPIO) for biomedical application as MRI contrast agents. Int J Nanomedicine.
6 Tanimoto A., Kuribayashi S. (2006). Application of superparamagnetic iron oxide to imaging of hepatocellular carcinoma. Eur J Radiol.
7 Maes R.M., Lewin J.S., Duerk J.L., Misselwitz B., Kiewiet C.J., Wacker F.K. (2006). A new type of susceptibility-artefact-based magnetic resonance angiography: intra-arterial injection of superparamagnetic iron oxide particles (SPIO) A Resovist in combination with TrueFisp imaging: a feasibility study. Contrast Media Mol Imaging.
8 Tanimoto A., Kuribayashi S. (2005). Hepatocyte-targeted MR contrast agents: contrast enhanced detection of liver cancer in diffusely damaged liver. Magn Reson Med Sci.
9 Montet X., Weissleder R., Josephson L. (2006). Imaging pancreatic cancer with a peptide-nanoparticle conjugate targeted to normal pancreas. Bioconjug Chem.
10 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
11 Reddy J.A., Allagadda V.M., Leamon C.P. (2005). Targeting therapeutic and imaging agents to folate receptor positive tumors. Curr Pharm Biotechnol.
12 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.